# [^11^C]Norepinephrine

Chemical name: | [^11^C]Norepinephrine
Abbreviated name: | [^11^C]NE
Synonym: | [^11^C]Norepinephrine hydrochloride, racemic [^11^C]norepinephrine
Agent Category: | Compound
Target: | Norepinephrine transporter (NET), vesicular monoamine transporter (VMAT), neuronal storage vesicle, monoamine oxidase (MAO), catechol-O-methyl transferase (COMT)
Target Category: | Transporter binding, storage and metabolism in the sympathetic nervous system (SNS)
Method of detection: | Positron Emission Tomography (PET)
Source of signal/contrast: | ^11^C
Activation: | No
Studies: | - Non–primate non-rodent mammals; - Non-human primates | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C-Norepinephrine%20OR%20%5B11C%5DNE)]

[^11^C]Norepinephrine ([^11^C]NE) is a radioligand developed for positron emission tomography (PET) imaging of the sympathetic nervous system (SNS). It is a catecholamine analog labeled with ^11^C, a positron emitter with a physical half-life (t_½_) of 20.4 min (1).

Many diseases affect the SNS, and imaging of pathologic changes of adrenergic transmission has been an important area of PET research (2, 3). Most postganglionic sympathetic neurons in the autonomic nervous system release the neurotransmitter norepinephrine (NE), which stimulates adrenergic receptors in various effector organs (4). There are different types of adrenergic receptors, and NE stimulates α_1_, β_1_, and certain β_2_ receptors. The NE transporter (NET) is a transmembrane protein located in the adrenergic nerve terminals that is responsible for active reuptake (uptake-1) of NE released from neurons (5). NE is stored in the neuronal vesicles and is released on stimulation. Significant expression of NET is found in major organs of the SNS such as the heart and brain. There is substantial evidence that aberrations in cardiac SNS function contribute to the morbidity and mortality associated with cardiac diseases (6).

Molecular probes with structures closely related to NE can be used to assess the integrity of presynaptic sympathetic nerve terminals in various diseases. [^123^I]meta-Iodobenzylguanidine ([^123^I]MIBG), a single-photon emission tomography (SPECT) agent, has been developed and used for neuronal imaging (7). Efforts have been made to develop a positron-emitting tracer because of the inadequate quantitative information and lower spatial resolution obtained by SPECT imaging with [^123^I]MIBG (7). Studies with [^14^C]NE and [^3^H]NE have shown that when radiolabeled NE was injected intravenously into animals, NE rapidly disappeared from the circulation and accumulated in organs rich in SNS (7, 8). NE is taken up by NET and transported by vesicular monoamine transporter into storage vesicles. However, radiolabeled NE is subject to metabolism by both monoamine oxidase and catechol-O-methyl transferase. Langer and Haldin (7) reviewed and compared various PET and SPECT trances for mapping the cardiac nervous system.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2811C-Norepinephrine%20OR%20%5B11C%5DNE%29%20AND%20synthesis)]

Racemic ^11^C-labeled NE ((±)-[^11^C]NE) was first synthesized by Fowler et al. (9). The synthetic approach was similar to the synthesis of [^11^C]dopamine. The synthesis of radiolabeled. NE is complicated by the presence of the stereogenic center generated by a β-hydroxyl group. In this synthesis (9, 10), [^11^C]NE was prepared by reduction of cyanohydrins with borane. Briefly, a mixture of sodium cyanide, 3,4-dihydroxybenzaldehyde, and sodium bisulfite was heated at 70 ºC for 30 min and then extracted with ether. After the ether was evaporated, a 1 M borane was added to the residue after the ether was evaporated and allowed to stand 5 min at room temperature. The NE hydrochloride was separated by Dowex 50 W-Xs chromatography with a yield of 14.2%. The radiosynthesis prepared Na[^11^C]CN from H[^11^C]CN and used Na[^11^C]CN in the same procedure to give a radiochemical yield of approximately 10% based on the initial activity of H[^11^C]CN at the end of bombardment (EOB).

Nagren et al. (11) used no-carrier-added [^11^C]nitromethane as the starting chemical to react with 3,4-(methylenedioxy)-benzaldehyde to produce [β-^11^C]3,4-(methylenedioxy)-β-nitrophenethyl alchol. This intermediate product was then reduced with Raney nickel in 30% formic acid to produce [^11^C]NE. The final product was purified by high-performance liquid chromatography (HPLC). [^11^C]Nitromethane was prepared from [^11^C]carbon dioxide by the ^14^N(p,α)^11^C reaction. The radiochemical yield was 20-25% (decay-corrected activity from [^11^C]CO_2_) with a total synthesis time of 65-75 min (from EOB to the final filtered product). The reported specific activity was 26-56 GBq(700-1500 Ci)/µmol. In another study, Nagren et al. (12) described the use of a preparative HPLC method for the separation of (−)- and (+)-[^11^C]NE.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2811C-Norepinephrine%20OR%20%5B11C%5DNE%29%20AND%20in%20vitro)]

No publication is currently available.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2811C-Norepinephrine%20OR%20%5B11C%5DNE%29%20AND%20rodentia)]

No publication is currently available.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2811C-Norepinephrine%20OR%20%5B11C%5DNE%29%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

Fowler et al. (9) evaluated the biodistribution of carrier-free, racemic [^11^C]NE in 4 dogs. The radioactivities in percentage of injected dose/gram of tissue, in the heart at 15, 30, 60, and 90 min after injection were 0.017, 0.023, 0.025, and 0.023, respectively. The heart/blood, heart/lung, heart/liver, heart/kidney, and heart/adrenal medulla ratios at 1 h were 11.04, 4.89, 2.28, 0.908, and 0.28, respectively. The biological t_½_ in the blood was less than 2 min.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2811C-Norepinephrine%20OR%20%5B11C%5DNE%29%20AND%20%28primate%20NOT%20human%29)]

Farde et al. (13, 14) studied the heart uptake of racemic [^11^C]NE with PET imaging in 2 cynomolgus monkeys. Racemic [^11^C]NE was prepared with a specific activity >37,000 GBq (1000 Ci)/mmol. A dose of 20-40 MBq (0.54-1.08 mCi at the time of administration) was injected intravenously into the monkey. After the injection, there was a rapid, high uptake of radioactivity by the heart. The radioactivity in the myocardium was more than 10 times higher than that in the adjacent lung tissue and 5 times more than that in the plasma. Following a 1-h pretreatment with desipramine (3 mg/kg i.v.; a reuptake inhibitor), the radioactivity of [^11^C]NE was reduced by 80-85%. This uptake inhibition probably indicated that a major proportion of the radioactivity represented binding and transport of this radioactive tracer by NET into the neuronal vesicles. More than 90% of plasma radioactivity represented unchanged ligand 30 min after injection (15).

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2811C-Norepinephrine%20OR%20%5B11C%5DNE%29%20AND%20human)]

No publication is currently available.

## NIH Support

NIMH Grant 42105-7.

## References

1 Rosenspire K.C., Haka M.S., Van Dort M.E., Jewett D.M., Gildersleeve D.L., Schwaiger M., Wieland D.M. (1990). Synthesis and preliminary evaluation of carbon-11-meta-hydroxyephedrine: a false transmitter agent for heart neuronal imaging. J Nucl Med.
2. Konishi, J., B.A. Dwamena, M.D. Gross, B. Shapiro, T. Misaki, M. Fukunaga, J.C. Sisson, H.-Y. Oei, M. De Jong, and E. P. Krenning Endocrinology, in Molecular Nuclear Medicine, L.E. Feinendegen, W.W. Shreeve, W.C. Eckelman, Y.-W. Bahk, and H.N. Wagner Jr., Editor. 2003, Springer: New York. p. 357-409.
3. Antoni, G., T. Kihlberg, and B. Langstrom, Aspects on the synthesis of 11C-Labelled compounds, in Handbook of Radiopharmaceuticals, M.J. Welch, and C.S. Redvanly, Editor. 2003, John Wiley & Sons Ltd.: West Sussex, England. p. 141-194.
4. Sunderland, P.M., Pathophysiology. The Biologic basis for disease in adults and children, K.L. McCance, and S. E. Huether, Editor. 1994, Mosby-Year Books, Inc.: St, Louiis. p. 397-436.
5 Buursma A.R., Beerens A.M., de Vries E.F., van Waarde A., Rots M.G., Hospers G.A., Vaalburg W., Haisma H.J. (2005). The Human Norepinephrine Transporter in Combination with 11C-m-Hydroxyephedrine as a Reporter Gene/Reporter Probe for PET of Gene Therapy. J Nucl Med.
6 Caldwell J.H., Kroll K., Li Z., Seymour K., Link J.M., Krohn K.A. (1998). Quantitation of presynaptic cardiac sympathetic function with carbon-11-meta-hydroxyephedrine. J Nucl Med.
7 Langer O., Halldin C. (2002). PET and SPET tracers for mapping the cardiac nervous system. Eur J Nucl Med Mol Imaging.
8 Su C., Bevan J.A., Osher J.V. (1972). A double-labeled frozen section technique for studying distribution of H 3 -norepinephrine. Experientia.
9 Fowler J.S., MacGregor R.R., Ansari A.N., Atkins H.L., Wolf A.P. (1974). Radiopharmaceuticals. 12. A new rapid synthesis of carbon-11 labeled norepinephrine hydrochloride. J Med Chem.
10. Fowler, J.S., A.P. Wolf, D.R. Christman, R.R. MacGregor, A.N. Ansari, and H. Atkins, Carrier-free 11C-labeled catecholamines, in Radiopharmaceuticals, G. Subramanian, B.A. Rhodes, J.F. Cooper, and V.J. Sodd, Editors. 1975, Society of Nuclear Medicine: New York. p. 196-204.
11 Nagren K., Schoeps K.O., Halldin C., Swahn C.G., Farde L. (1994). Selective synthesis of racemic 1-11C-labelled norepinephrine, octopamine, norphenylephrine and phenylethanolamine using [11C]nitromethane. Appl Radiat Isot.
12 Nagren K., Halldin C., Lundkvist C., Eriksson A., Farde L. (1996). HPLC separation of (-)-(L)- and (+)-(D)-[C-11]norepinephrine for preclinical PET examinations. Eur J Nucl Med.
13 Farde L., Halldin C., Nagren K., Suhara T., Karlsson P., Schoeps K.O., Swahn C.G., Bone D. (1994). Positron emission tomography shows high specific uptake of racemic carbon-11 labelled norepinephrine in the primate heart. Eur J Nucl Med.
14 Farde L., Halldin C., Nagren K., Karlsson P., Swahn C.G., Suhara T. (1995). PET examination of the monkey heart with high specific radioactivity [11C]norepinephrine and [11C]metaraminol. Nucl Med Biol.
15 Swahn C.G., Halldin C., Nagren K., Farde L. (1995). An HPLC-method for determination of ligand metabolism during PET studies with [11C]metaraminol and [11C]norepinephrine. Nucl Med Biol.